# ^111^In-Labeled Ac-Phe-Lys(DTPA)-Tyr-Lys(DTPA)-NH_2_ (IMP-156)

Chemical name: | 111In-Labeled Ac-Phe-Lys(DTPA)-Tyr-Lys(DTPA)-NH2 (IMP-156)
Abbreviated name: | [111In]-IMP-156
Synonym:
Agent Category: | Compound
Target: | Bispecific PAM4 antibody
Target Category: | Antibody
Method of detection: | Single photon emission computed tomography (SPECT); gamma planar imaging
Source of signal / contrast: | 111In
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=PAM4&cmd=DetailsSearch)]

The majority of individuals suffering from pancreatic adenocarcinoma (PAC) do not survive for more than 1 year after diagnosis and fewer than 1% of these patients live beyond 5 years (1). Although surgical resection of the cancer is a possible intervention for this disease only 10 – 25% of the patients are considered suitable for this treatment because usually by the time that neoplasm is detected the malignancy has metastasized to other organs and the tumor load in the patient is too high to warrant surgery (1). Patients with nonresectable PAC are treated either with gemcitabine (http://www.cancer.gov/cancertopics/druginfo/gemcitabinehydrochloride) or radiotherapy or a combination of the two, however, these treatments are not curative because they only prolong survival and improve the quality of life of the patient during that time (1). The detection of this cancer at an early stage can facilitate proper staging of the disease so that a suitable treatment regimen can be initiated to possibly improve patient prognosis (2). In this regard the monoclonal antibody (mAb), PAM4, which specifically targets mucin 1 (MUC1), a glycoprotein, overexpressed only in PAC tumors was developed, radiolabeled with ^131^I or ^111^In and shown to detect neoplastic tumors with scintigraphy in patients having pancreatic malignancies (3). However, intact radiolabeled antibodies are of limited utility to visualize cancerous lesions due to their large size (~150 kDa) and long circulating half-life (4). To amplify the signal obtained from an radiolabeled agent that can be used to detect or treat malignant tumors noninvasively, investigators have developed and evaluated a variety of strategies in preclinical studies in animals such as pretargeting the cancer lesion with a suitable mAb (or its derivative) followed by exposing the animals to an appropriate radiolabeled small molecular weight ligand that targets the mAb or its derivative. This technique has been shown to generate a higher signal-to-noise ratios during imaging compared to ratios obtained with a directly labeled mAb alone (5-7). Use of the pretargeting technique for the imaging and therapy of cancer has been discussed in detail elsewhere (8, 9).

Cardillo et al. developed a bispecific F(ab’)_2_ mAb (bsPAM4; bsmAb) by cross-linking a PAM4 Fab’ fragment (binds the MUC-1 antigen) to a murine anti-indium-diethylenetriaminepentaacetic acid (DTPA) mAb Fab’ fragment (binds the peptide hapten antigen) and used the unlabeled bsmAb to pretarget human CaPan-1 cell xenograft PAC tumors in nude mice (3). After the bsmAb was cleared from blood circulation the animals were injected with a radiolabeled peptide hapten to visualize the PAC lesions by whole body scintigraphy. To confirm the tumor targeting specificity bsPAM4 (the pretargeting bsmAb) the biodistribution of this bsmAb was investigated with ^125^I-labeled bsPAM4 ([^125^I]-bsPAM4) in mice bearing human PAC tumors (3). Subsequently two groups of animals pretargeted with bsPAM4 were separately injected with radiolabeled peptide haptens, ^111^In-labeled Ac-Phe-Lys(DTPA)-Tyr-Lys(DTPA)-NH_2_ ([^111^In]-IMP-156) and ^99^Tc-labeled Ac-Lys(DTPA)-Tyr-Lys(DTPA)-Lys(thiosemicarbazonyl-glyoxyl-cysteinyl-)-NH_2_ ([^99m^Tc]-IMP-192), and the biodistribution of these radiolabeled peptides was investigated in the tumor bearing rodents. This chapter describes the biodistribution and imaging studies performed with [^111^In]-IMP-156. The biodistribution of radioiodinated bsPAM4 in non-pretargeted mice (10) and the biodistribution of [^99m^Tc]-IMP-192 in mice pretargeted with bsPAM4 (11) are discussed in separate chapters of MICAD (www.micad.nih.gov).

### Other Sources of Information

Peptide haptens [PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=peptide%20haptens&cmd=DetailsSearch)]

Clinical trials (http://clinicaltrials.gov/ct2/results?term=bispecific+antibody) with bispecific antibodies

Application of multivalent antibodies [PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=application%20of%20multivalent%20antibodies&cmd=DetailsSearch)]

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=125I-bsPAM4%20synthesis&cmd=DetailsSearch)]

The synthesis of bsPAM4 and bispecific retuximab (bsRIT; for use as a control) has been described by Cardillo et al. (3). The cross-linked bsmAbs were purified by size-exclusion chromatography (SEC) and the ratio of each Fab’ fragment in the complex was determined to be 1:1 with high performance liquid chromatography. The two bsmAbs were labeled with ^125^I using the chloramine-T method to obtain [^125^I]-bsPAM4 and [^125^I]-bsRIT as described elsewhere (3). [^125^I]-bsPAM4 and [^125^I]-bsRIT were reported to have specific activities (SA) of 492.2 MBq/mg (11.6 mCi/mg) and 403.3 MBq/mg (10.9 mCi/mg), respectively. The radiochemical purity and yield of the radioiodinated bsmAbs was not reported.

In an imaging study [^111^In]-labeled chimeric PAM4 (cPAM4) with a SA of 32.6 MBq/mg (0.88 mCi/mg was used as a control (3). The radiochemical yield and purity of this labeled antibody was not reported.

IMP-156 was obtained from a commercial source and labeled with ^111^In after chelation with diethylenetriamine pentaacetic acid (DTPA) and the residual DTPA sites on the peptide were quenched by the addition of nonradioactive indium (3). The number of indium atoms bound to each IMP-156 molecule (that has two DTPA sites within the structure as described above) was not reported. The SA of [^111^In]-IMP-156 was reported to be 183.2 MBq/nmol (4.95 mCi/nmol) and the radiolabeled peptide was reported to contain no aggregates and <2% unbound radioactivity as determined by instant thin layer chromatography.

The peptide hapten IMP-192 was obtained from the same commercial source as that of IMP-156 and labeled with ^99m^Tc as described by Cardillo et al. (3). The SA of [^99m^Tc]-IMP-192 was 77.7 MBq/nmol (2.1 mCi/nmol) and the amount of aggregates and the unbound radioactivity content was the same as the [^111^In]-IMP-156 preparation mentioned above. In an earlier study the radiochemical yield of the ^99m^Tc-labeled peptide hapten was reported to be 94-99% with a SA of up to 67.7 GBq/mmol (1.83 Ci/mmol).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=IMP-192%20in%20vitro&cmd=DetailsSearch)]

Karacay et al. reported that both IMP-156 and IMP-192 can be stored in a freeze dried form at -20^o^ C for prolonged periods (12).

In a study to investigate the bsmAb binding characteristics of [^111^In]-IMP-156, 0.15 pmol of the labeled peptide was mixed with 10 pmol bsPAM4 in presence of excess MUC1 (200 μg) and the mixture was incubated at 37^o^ C for 1 h (3). Subsequently, size-exclusion chromatography (SEC) of the mixture revealed that 88% of the tracer bound to bsPAM4. Of the total bsmAb bound fraction 92% of the label was in the MUC1 fraction, 6% in the non-MUC1-reactive bsPAM4 fraction and 2% of the radiocompound bound nonspecifically to the MUC1 antigen.

The in vitro stability of [^99m^Tc]-IMP-192 in normal saline (0.9% sodium chloride), 1% human serum albumin and 10 mM cysteine was reported to be 96%, 96% and 89%, respectively, as determined by reversed-phase high performance liquid chromatography (12).

The bsmAb binding characteristics of [^99m^Tc]-IMP-192 were also studied as described above (3). An analysis of the mixture with SEC showed that 81% of this tracer was bound to bsPAM4 and of the total fraction bound to bsmAb 85% of the label eluted in the MUC1 fraction, 11% in the non-MUC1-reactive bsPAM4 fraction and 4% of the radiocompound bound nonspecifically to the MUC1 antigen.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=125I-bsPAM4%20rodentia&cmd=DetailsSearch)]

The biodistribution of [^111^In]-IMP-156 was investigated in athymic nu/nu mice bearing human PAC CaPan-1 cell tumors (n = 14 mice/group) pretargeted with either [^125^I]-bsPAM4 or [^125^I]-bsRIT (control bsmAb) (3). A group of animals was injected with 10 μCi (150 pmol) [^125^I]-bsPAM4 and two other groups received 10 μCi (150 pmol) [^125^I]-bsRIT. Two other groups of animals received the labeled peptides alone. After 40 h a group mice were injected with 35 μCi (15 pmol) [^111^In]-IMP-156 and the animals were euthanized at 3 and 24 h post injection (p.i.; i. e. 43 and 64 h after administration of the bsmAbs). All organs of interest, including the tumors, were removed from the mice and the amount of radioactivity in the various tissues was determined. Data obtained from this study was presented as percent of injected dose per gram tissue (%ID/g). The biodistribution of [^99m^Tc]-IMP-192 was also investigated in the animals as described above (3). No blocking studies were reported with either labeled peptide hapten.

At 3 h after injecting ^111^In-labeled IMP-156 the amount of radioactivity in the tumor from animals pretreated with bsPAM4 was determined to be 20.2 ± 5.5%ID/g (P < 0.0001) compared to 0.9 ± 0.1%ID/g in tumors of the bsRIT pretreated animals (3). With [^99m^Tc]-IMP-192 the amount of radioactivity in the tumors of bsPAM4 and bsRIT pretargeted animals were reported to be 16.8 ± 4.8%ID/g (P < 0.0005) and 1.1 ± 0.2%ID/g, respectively. Both the radiolabeled peptides were shown to clear rapidly from the body of the non-pretargeted animals.

At 24 h after the treatment with [^111^In]-IMP-156 tumors from mice pretreated with bsPAM4 had a radioactivity uptake of 11.1 ± 3.5%ID/g (P < 0.0008) compared to 0.5 ± 0.02%ID/g in animals pretreated with bsRIT (3). In comparison, with [^99m^Tc]-IMP-192 the tumors from animals pretargeted with bsPAM4 and bsRIT showed an accumulation of 12.9 ± 4.2%ID/g (P < 0.0008) and 0.4 ± 0.03%ID/g, respectively, at the same time point.

At 24 h after treatment with either [^111^In]-IMP-156 or [^99m^Tc]-IMP-192 the tumor-to-nontumor ratios for all tissues obtained from animals pretargeted with bsPAM4 were higher than those obtained from non-pretargeted animals treated with [^125^I]-bsPAM4 alone (the P value range was <0.0001 to 0.008) (3).

In the animals pretreated with bsPAM4 the tumor-to-blood ratio with [^111^In]-IMP-156 and [^99m^Tc]-IMP-192 were 274:1 and 80:1, respectively, compared to a ratio of 4:1 obtained with the non-pretargeted mice injected with [^125^I]-bsPAM4 alone (P<0.0002).

For imaging studies athymic mice bearing CaPan-1 xenograft tumors (n = 2 animals/group) were pretargeted with bsPAM4 and 40 h later injected with [^111^In]-IMP-156 (3). The control group was administered bsRIT followed an injection of the ^111^In-labeled peptide. Another group of animals received an injection of only [^111^In]-IMP-156 and the last group was injected with only [^111^In]-cPAM4 IgG. The whole body clearance of radioactivity from [^111^In]-IMP-156 was reported to be >85% at 4 h post injection (p.i.) compared to only 18% with the labeled cPAM4 IgG. The tumors were visible in the pretargeted animals at 0.5 h p.i. and remained visible with little background activity even at 24 to 168 h p.i. indicating that the radiolabeled peptide bound specifically to the tumors and was retained in the lesions during this period. Although tumors were also visible in animals injected with the directly labeled cPAM4 a high background activity was observed in the abdominal regions of the animals. No tumors were visualized by scintigraphy of animals pretargeted with bsRIT or mice treated with the labeled peptides alone (3).

From these studies the investigators concluded that both [^111^In]-IMP-156 and [^99m^Tc]-IMP-192 were suitable to detect PAC xenograft tumors pretargeted with bsPAM4 in rodents (3).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=111In-IMP-156%20Other%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=111In-IMP-156%20Non-Human%20Primates&cmd=DetailsSearch)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=111In-IMP-156%20Human%20Studies&cmd=DetailsSearch)]

No publication is currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## NIH Support

Studies described in this chapter were supported by National Institutes of Health grants CA-54425 and CA92723.

## References

1 Gold D.V., Cardillo T., Goldenberg D.M., Sharkey R.M. (2001). Localization of pancreatic cancer with radiolabeled monoclonal antibody PAM4. Crit Rev Oncol Hematol.
2 Gold D.V., Goggins M., Modrak D.E., Newsome G., Liu M., Shi C., Hruban R.H., Goldenberg D.M. (2010). Detection of early-stage pancreatic adenocarcinoma. Cancer Epidemiol Biomarkers Prev.
3 Cardillo T.M., Karacay H., Goldenberg D.M., Yeldell D., Chang C.H., Modrak D.E., Sharkey R.M., Gold D.V. (2004). Improved targeting of pancreatic cancer: experimental studies of a new bispecific antibody, pretargeting enhancement system for immunoscintigraphy. Clin Cancer Res.
4 Ahlgren S., Orlova A., Wallberg H., Hansson M., Sandstrom M., Lewsley R., Wennborg A., Abrahmsen L., Tolmachev V., Feldwisch J. (2010). Targeting of HER2-expressing tumors using 111In-ABY-025, a second-generation affibody molecule with a fundamentally reengineered scaffold. J Nucl Med.
5 Forster G.J., Santos E.B., Smith-Jones P.M., Zanzonico P., Larson S.M. (2006). Pretargeted radioimmunotherapy with a single-chain antibody/streptavidin construct and radiolabeled DOTA-biotin: strategies for reduction of the renal dose. J Nucl Med.
6 Liu G., Dou S., Pretorius P.H., Liu X., Chen L., Rusckowski M., Hnatowich D.J. (2010). Tumor pretargeting in mice using MORF conjugated CC49 antibody and radiolabeled complimentary cMORF effector. Q J Nucl Med Mol Imaging.
7 Uppal J.K., Varshney R., Hazari P.P., Chuttani K., Kaushik N.K., Mishra A.K. (2011). Biological evaluation of avidin-based tumor pretargeting with DOTA-Triazole-Biotin constructed via versatile Cu(I) catalyzed click chemistry. J Drug Target.
8 Goldenberg D.M., Sharkey R.M. (2010). Radioactive antibodies: a historical review of selective targeting and treatment of cancer. Hosp Pract (Minneap).
9 Sharkey R.M., Goldenberg D.M. (2011). Cancer radioimmunotherapy. Immunotherapy.
10 Chopra, A., 125I-Labeled anti-mucin 1 bispecific antibody bsPAM4. Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.
11 Chopra, A., 99Tc-labeled Ac-Lys(DTPA)-Tyr-Lys(DTPA)-Lys(thiosemicarbazonyl-glyoxyl-cysteinyl-)-NH2 (IMP-192). Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.
12 Karacay H., McBride W.J., Griffiths G.L., Sharkey R.M., Barbet J., Hansen H.J., Goldenberg D.M. (2000). Experimental pretargeting studies of cancer with a humanized anti-CEA x murine anti-[In-DTPA] bispecific antibody construct and a (99m)Tc-/(188)Re-labeled peptide. Bioconjug Chem.